# ^68^Ga-1,4,7-Triazacyclononane,1-glutaric acid-4,7-acetic acid-p-Cl-Phe-cyclo(D-Cys-Tyr-D-4-amino-Phe(carbamoyl)-Lys-Thr-Cys)D-Tyr-NH_2_

Chemical name: | ^68^Ga-1,4,7-Triazacyclononane,1-glutaric acid-4,7-acetic acid-p-Cl-Phe-cyclo(D-Cys-Tyr-D-4-amino-Phe(carbamoyl)-Lys-Thr-Cys)D-Tyr-NH_2_
Abbreviated name: | ^68^Ga-NODAGA-LM3
Synonym:
Agent category: | Peptide
Target: | Somatostatin receptor (sst2)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=47117741), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=71979669) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6750) for more information about somatostatin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-LM3)]

Somatostatin (SST) is an inhibitor of the release of somatotropin, glucagon, insulin, gastrointestinal hormones, and other secretory proteins (1). SST is also known as somatotropin release-inhibiting factor (SRIF). SST is a cyclic polypeptide with two biologically active isoforms, SRIF-14 and SRIF-28, of 14 and 28 amino acids, respectively. SRIF has a short plasma half-life of <3 min (2). SST receptors (SSTRs) (G-protein–coupled) have been found on a variety of neuroendocrine tumors and cells of the immune system, and five individual subtypes (SSTR1–SSTR5) have been identified and subsequently cloned from animal and human tissues (3, 4). SST also inhibits cell proliferation and promotes apoptosis through binding to specific cell-surface SSTRs (5).

^111^In-Diethylenetriamine pentaacetic acid-octreotide (^111^In-DTPA-OCT) is an SST analog that, over the last decade, has remained the most widely used radiopharmaceutical for the scintigraphic detection and staging of primary and metastatic neuroendocrine tumors bearing SSTRs and the only FDA approved radiotracer with single-photon emission computed tomography (SPECT) (6). It has also shown promising results in peptide-receptor radionuclide therapy (7). Octreotide (OCT) is a cyclic peptide with eight amino acids. ^111^In-DTPA-OCT binds with high affinity to SSTR2 and SSTR5 and to SSTR3 to a lesser degree, but it does not bind to SSTR1 and SSTR4 (8). A large number of radiolabeled SST analogs have been reported using different radionuclides and different linkers. Currently used targeting SSTR peptides are mainly SSTR2 agonists. Therefore, there is a need for SSTR2 antagonist radioligands (9). p-Cl-Phe-cyclo(D-Cys-Tyr-D-4-amino-Phe(carbamoyl)-Lys-Thr-Cys)D-Tyr-NH_2_ (LM3) is a novel selective SSTR2 antagonist. Fani et al. (10) prepared ^68^Ga-1,4,7-triazacyclononane,1-glutaric acid-4,7-acetic acid-LM3 (^68^Ga-NODAGA-LM3) as a positron emission tomography (PET) imaging agent for SSTR2.

### Related Resource Links:

- Chapters in MICAD (Somatostatin (http://www.ncbi.nlm.nih.gov/books?term=Somatostatin%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (Somatostatin (http://www.ncbi.nlm.nih.gov/gene/6750), SSTR2 (http://www.ncbi.nlm.nih.gov/gene/6752))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Somatostatin (http://omim.org/entry/182450), SSTR2 (http://omim.org/entry/182452))
- Clinical trials (Somatostatin receptor (http://www.clinicaltrials.gov/ct2/results?term=somatostatin+receptor))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-LM3+and+synthesis)]

NODAGA-LM3 was synthesized via standard solid-phase peptide synthesis with a calculated mass of 1,522.6 Da in agreement with mass spectrometry (10). NODAGA was incorporated at the N-terminus of the peptide. NODAGA-LM3 was purified with high-performance liquid chromatography. ^68^Ga was complexed to NODAGA-LM3 by reaction of NODAGA-LM3 with ^68^Ga in sodium acetate (pH 4.0) for 10 min at room temperature. ^68^Ga-NODAGA-LM3 had a >95% radiochemical purity and specific activity of 120 MBq/nmol (3.2 mCi/nmol), with a labeling yield >97%. ^68^Ga-NODAGA-LM3 had a log D value of –2.33 ± 0.22 and a net charge of +1.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-LM3+and+in+vitro)]

Fani et al. (10) reported that ^nat^Ga-NODAGA-LM3 had 50% inhibition concentration (IC_50_) values of >1,000, 1.3 ± 0.3, >1,000, >1,000, and >1,000 nM for human SSTR1, SSTR2, SSTR3, SSTR4, and SSTR5 receptors in competition with ^125^I-SRIF-28, respectively. Immunofluorescence studies showed that the agonist [Tyr^3^]octreotide (10 nM) triggers receptor internalization whereas ^nat^Ga-NODAGA-LM3 at a much higher concentration (1,000 nM) does not stimulate receptor internalization in HEK-sst2 cells. ^nat^Ga-NODAGA-LM3 was able to inhibit receptor internalization induced by [Tyr^3^]octreotide.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-LM3+and+rodentia)]

Fani et al. (10) performed ex vivo biodistribution studies with 13.0 MBq (0.35 mCi) ^68^Ga-NODAGA-LM3 in nude mice (n = 3) bearing HEK-sst2 xenografts at 1 h after injection. The accumulation of radioactivity in the SSTR2 tumor was 37.27 ± 5.49% injected dose per gram (% ID/g). The kidney had the highest accumulation (19.68% ID/g), followed by the pancreas (9.15% ID/g), stomach (5.36% ID/g), lung (3.01% ID/g), adrenal (2.55% ID/g), bone (2.31% ID/g), and liver (1.08% ID/g). Accumulation of radioactivity in the other tissues was low, and the concentration in the blood was 0.91% ID/g. The tumor/blood, tumor/liver, tumor/kidney, and tumor/muscle ratios were 41.1, 34.7, 1.9, and 104.8, respectively. ^68^Ga-NODAGA-LM3 accumulation in the kidney was 1-fold higher than that of ^64^Cu-NODAGA-LM3 at 1 h after injection, and tumor accumulation at 1 h after injection was similar for both agents. ^68^Ga-NODAGA-LM3 exhibited 30% higher tumor and 65% lower kidney accumulation than ^68^Ga-DOTA-LM3. No blocking studies were reported.

Whole-body PET imaging (n=1) visualized the SSTR2 tumor at 1 h after injection of 6 MBq (0.16 mCi) ^68^Ga-NODAGA-LM3. The visualization was abrogated by co-injection of excess unlabeled peptide.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-LM3+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-LM3+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA-LM3+and+human)]

No publication is currently available.

## References

1 Weckbecker G., Lewis I., Albert R., Schmid H.A., Hoyer D., Bruns C. (2003). Opportunities in somatostatin research: biological, chemical and therapeutic aspects. Nat Rev Drug Discov.
2 Patel Y.C., Wheatley T. (1983). In vivo and in vitro plasma disappearance and metabolism of somatostatin-28 and somatostatin-14 in the rat. Endocrinology.
3 Corleto V.D., Nasoni S., Panzuto F., Cassetta S., Delle Fave G. (2004). Somatostatin receptor subtypes: basic pharmacology and tissue distribution. Dig Liver Dis.
4 Moller L.N., Stidsen C.E., Hartmann B., Holst J.J. (2003). Somatostatin receptors. Biochim Biophys Acta.
5 Barnett P. (2003). Somatostatin and somatostatin receptor physiology. Endocrine.
6 Krenning E.P., Kwekkeboom D.J., Bakker W.H., Breeman W.A., Kooij P.P., Oei H.Y., van Hagen M., Postema P.T., de Jong M., Reubi J.C., et al. (1993). Somatostatin receptor scintigraphy with [111In-DTPA-D-Phe1]- and [123I-Tyr3]-octreotide: the Rotterdam experience with more than 1000 patients. Eur J Nucl Med.
7 Kwekkeboom D.J., Mueller-Brand J., Paganelli G., Anthony L.B., Pauwels S., Kvols L.K. (2005). M. O'Dorisio T, R. Valkema, L. Bodei, M. Chinol, H.R. Maecke, and E.P. Krenning, Overview of results of peptide receptor radionuclide therapy with 3 radiolabeled somatostatin analogs. J Nucl Med.
8 Storch D., Behe M., Walter M.A., Chen J., Powell P., Mikolajczak R., Macke H.R. (2005). Evaluation of [99mTc/EDDA/HYNIC0]octreotide derivatives compared with [111In-DOTA0,Tyr3, Thr8]octreotide and [111In-DTPA0]octreotide: does tumor or pancreas uptake correlate with the rate of internalization?. J Nucl Med.
9 Reubi J.C., Schar J.C., Waser B., Wenger S., Heppeler A., Schmitt J.S., Macke H.R. (2000). Affinity profiles for human somatostatin receptor subtypes SST1-SST5 of somatostatin radiotracers selected for scintigraphic and radiotherapeutic use. Eur J Nucl Med.
10 Fani M., Del Pozzo L., Abiraj K., Mansi R., Tamma M.L., Cescato R., Waser B., Weber W.A., Reubi J.C., Maecke H.R. (2011). PET of somatostatin receptor-positive tumors using 64Cu- and 68Ga-somatostatin antagonists: the chelate makes the difference. J Nucl Med.